# Cypate-Gly-Arg-Asp-Ser-Pro-Lys

Chemical name: | Cypate-Gly-Arg-Asp-Ser-Pro-Lys
Abbreviated name: | Cyp-GRD, Cyp-GRDSPK
Synonym:
Agent category: | Peptide
Target: | α_v_β_3_ integrin
Target category: | Receptor binding
Method of detection: | Optical, near-Infrared fluorescence (NIR) imaging
Source of signal: | Cypate
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%5BAll%20Fields%5D%20AND%20GRD%5BAll%20Fields%5D)]

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (8, 9), and the agonists are being studied as angiogenic agents for coronary angiogenesis (10, 11). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) is identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_. Various radiolabeled antagonists and peptides were introduced for imaging of tumors and tumor angiogenesis (12).

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (13-15). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700-1000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive complement to radionuclide imaging.

Cypate is a reactive carbocyanine dye, which is derived from indocyanine green (ICG) (16). Cypate was previously conjugated to octreotate (Cyp-OC). Cyp-OC was not toxic to rats up to 10 μmol/kg (17). From the results of investigating a small library of RGD peptides for their binding activity to the α_v_β_3_ integrin, a linear hexapeptide, Gly-Arg-Asp-Ser-Pro-Lys (GRDSPK), lacking the RGD sequence was conjugated with Cypate as Cyp-GRD to study in vivo biodistribution of the tracer in tumor-bearing mice (18). Cypate is a NIR fluorescent dye with an absorbance maximum at 778 nm and an emission maximum at 805 nm with a high extinction coefficient of 224,000 (mol/L)−^1^cm−^1^. Cyp-GRD was found to have a high and long-lasting accumulation in α_v_β_3_-positve A549 human non-small cell lung carcinomas in nude mice. The binding of Cyp-GRD to the integrin receptor was found to be specific both in vitro and in vivo.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%5BAll%20Fields%5D%20AND%20GRD%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

A detailed synthesis of Cypate was reported by Ye et al. (16). Cypate was conjugated to peptides prepared on solid support by standard fluorenylmethoxycarbonyl peptide synthesis (18). The conjugated peptides were subsequently cleaved from the solid resin and purified by high-performance liquid chromatography (HPLC) in good yields and high purity (>95%).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%5BAll%20Fields%5D%20AND%20GRD%20and%20In%20vitro)]

A549 cells were validated to have α_v_ and β_3_ integrins by immunohistochemistry and Western blot analysis (18). The β_3_ subunit was expressed at a higher level than the α_v_ subunit, suggesting that β_3_ may also be associated with another α subunit.

Fluorescence microscopy was used to study cellular distribution of Cyp-GRD in A549 cells (18). Cyp-GRD (1 μM) was internalized into the cytoplasm and not the nucleus by the cells at 37º C after 30 min of incubation, whereas the tracer remained on the cell surface at 4º C. The binding of the Cyp-GRD was inhibited by 10 μM cyclo(Arg-Gly-Asp-D-Phe-Val), an RGD antagonist with little fluorescence that was visible in A549 cells. The binding and internalization of Cyp-GRD were also inhibited by anti-β_3_ antibody (10 μM) and to a lesser extent by anti-α_v_ antibody (10 μM), suggesting an important role for the β_3_ subunit in the binding and internalization of Cyp-GRD in A549 cells. Cyp-GRD was not toxic to A549 cells up to 100 μM as measured by MTT (3-(4,5-dimethylthiazol-2-yl)-2,5-diphenyltetrazolium bromide) assay.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%5BAll%20Fields%5D%20AND%20GRD%20and%20rodentia)]

Biodistribution studies of Cyp-GRD were evaluated in nude mice bearing an A549 subcutaneous xenograft model (18). Whole-body small animal images by reflectance planar fluorescence were obtained at various time points after injection of Cyp-GRD (0.3 μmol/kg). The tumor uptake of Cyp-GRD was visible at 8 h after the tracer had been cleared from the blood and non-targeted tissues. A maximal uptake in the tumor was reached at 24 h. The tracer uptake in the tumor could be blocked (>80%) by co-injection of cyclo(Arg-Gly-Asp-D-Phe-Val) (0.3 μmol/kg), whereas the blocking resulted in higher fluorescence intensity in the liver and kidneys. Use of an optical technique provided noninvasive imaging of tumor cells in mice.

The biodistribution of Cyp-GRD, Cypate-Gly-Arg-Gly-Asp-Ser-Pro-Lys (Cyp-RGD), and Cypate-cyclo(Arg-Gly-Asp-D-Phe-Val-Lys) (Cyp-cyclo-RGD) was studied in A549 tumor-bearing mice by ex vivo tissue fluorescence intensity measurements at 24 h after injection (18). Cyp-GRD uptake in tumor was the highest, followed to a lesser extent by Cyp-cyclo-RGD. The uptake of Cyp-RGD in the tumor was minimal. Cyp-cyclo-RGD and Cyp-RGD were markedly retained in the liver and kidneys as compared with Cyp-GRD. Cyp-GRD had a minimal uptake in non-targeted tissues. Furthermore, ^111^In-DOTA-GRD was not retained by the tumor. Therefore, there seems to be a synergic effect of Cypate- and GRD-containing peptide for binding to the α_v_β_3_ integrin.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%20GRD%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%20and%20GRD%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cypate%20and%20GRD%20AND%20human)]

No publication is currently available.

## NIH Support

R01 CA109754-01, R01 CA109754-02, R01 CA109754-03, R01CA109754, R21 CA100972-01, R33 CA100972-02, R33 CA100972-04, R33 CA100972

## References

1 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
2 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
5 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
6 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
7 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Sadeghi M.M., Krassilnikova S., Zhang J., Gharaei A.A., Fassaei H.R., Esmailzadeh L., Kooshkabadi A., Edwards S., Yalamanchili P., Harris T.D., Sinusas A.J., Zaret B.L., Bender J.R. (2004). Detection of injury-induced vascular remodeling by targeting activated alphavbeta3 integrin in vivo. Circulation.
11 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
12 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
13 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
14 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
15 Ntziachristos V., Schellenberger E.A., Ripoll J., Yessayan D., Graves E., Bogdanov A., Josephson L., Weissleder R. (2004). Visualization of antitumor treatment by means of fluorescence molecular tomography with an annexin V-Cy5.5 conjugate. Proc Natl Acad Sci U S A.
16 Ye Y., Bloch S., Kao J., Achilefu S. (2005). Multivalent carbocyanine molecular probes: synthesis and applications. Bioconjug Chem.
17 Achilefu S., Dorshow R.B., Bugaj J.E., Rajagopalan R. (2000). Novel receptor-targeted fluorescent contrast agents for in vivo tumor imaging. Invest Radiol.
18 Achilefu S., Bloch S., Markiewicz M.A., Zhong T., Ye Y., Dorshow R.B., Chance B., Liang K. (2005). Synergistic effects of light-emitting probes and peptides for targeting and monitoring integrin expression. Proc Natl Acad Sci U S A.